# ^111^In-BZ-Diethylenetriaminepentaacetic acid-Z_EGFR:1907_

^111^In-BZ-DTPA-Z_EGFR:1907_

Chemical name: | ^111^In-BZ-Diethylenetriaminepentaacetic acid-Z_EGFR:1907_
Abbreviated name: | ^111^In-BZ-DTPA-Z_EGFR:1907_
Synonym:
Agent category: | Antibody
Target: | EGFR
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT)
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about EGFR.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907)]

Epidermal growth factor (EGF) is a cytokine composed of 53 amino acids (6.2 kDa) that is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). Trastuzumab is approved for clinical use for anti-cancer therapies in both Europe and North America. ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab -F(ab')_2_ have been developed for imaging human breast cancer (12-16). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab´)_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 based on the Z-domain residues (58 amino acids) from one of the IgG-binding domains of staphylococcal protein A was constructed (17). Affibody molecules exhibit high binding affinity to HER2 with K_d_ values <100 pM. Various radiolabeled Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. Recently, the EGFR-specific Affibody Z_EGFR:1907_ (8.1 kDa) was identified and labeled with ^111^In via isothiocyanate-BZ-diethylenetriaminepentaacetic acid (DTPA) to form ^111^In-BZ-DTPA-Z_EGFR:1907_ for single-photon emission computed tomography (SPECT) imaging in nude mice bearing human tumors (18).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR+1907+synthesis)]

Isothiocyanate-BZ-DTPA and Z_EGFR:1907_ (1:1 molar ratio) were incubated in sodium borate buffer (pH 9) for 20 h at 37°C (18). BZ-DTPA-Z_EGFR:1907_ was isolated from the incubation mixture with a NAP-5 column with 95% coupling efficiency. BZ-DOTA- Z_EGFR:1907_ in 0.2 M ammonium acetate buffer (pH 5.25) was mixed with a predetermined amount of ^111^InCl_3_. The mixture was incubated for 1 h at room temperature with a labeling efficiency of >95%. ^111^In-BZ-DTPA-Z_EGFR:1907_ was purified with NAP-5 chromatography with a radiochemical purity of >95%. The specific activity of ^111^In-BZ-DTPA-Z_EGFR:1907_ was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20in%20vitro)]

In vitro binding specificity tests showed that binding of ^111^In-BZ-DTPA-Z_EGFR:1907_ to A431 cells expressing EGFR was mediated by the receptors because saturation of receptors by preincubation with non-labeled Z_EGFR:1907_ significantly decreased binding of ^111^In-BZ-DTPA-Z_EGFR:1907_ (18). The cell-bound radioactivity remained at 35–42% of the initially bound activity for up to 24 h. AlexaFluor 488-Z_EGFR:1907_ exhibited a K_d_ value of 2.8 nM for the EGFR of A431 cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20rodentia)]

Tolmachev et al. (18) performed biodistribution studies of ^111^In-BZ-DTPA-Z_EGFR:1907_ in nude mice (n = 4/group) bearing A431 xenografts. The tracer accumulation in the tumors was 3.7% injected dose per gram (ID/g) at 4 h and 2.0% ID/g at 24 h after injection. The organ with the highest radioactivity was the kidney (136 and 102% ID/g at 4 and 24 h, respectively), followed by the liver (5.0 and 1.2% ID/g at 4 and 24 h, respectively) and intestines (3.6 and 1.2% ID/g at 4 and 24 h, respectively). The radioactivity levels were low in the other organs and tissues. Blood levels were 1.5% ID/g at 1 h and 0.07% ID/g at 24 h. Tumor/blood ratios were 2.5 and 28.6 at 4 and 24 h after injection, respectively. Accumulation of control ^111^In-BZ-DTPA-Z_Taq_ Affibody in the tumors was only 0.4% ID/g at 4 h after injection, with high accumulation (189% ID/g) in the kidneys. SPECT gamma imaging analysis was performed in nude mice bearing A431 tumors after intravenous injection of ^111^In-BZ-DTPA-Z_EGFR:1907_. The tumors were clearly visualized at 24 h along with the kidneys. The tumor/muscle ratio was 6.8. No blocking experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Tolmachev V., Friedman M., Sandstrom M., Eriksson T.L., Rosik D., Hodik M., Stahl S., Frejd F.Y., Orlova A. (2009). Affibody molecules for epidermal growth factor receptor targeting in vivo: aspects of dimerization and labeling chemistry. J Nucl Med.